# Ultrasmall near-infrared gold nanoclusters

Chemical name: | Ultrasmall near-infrared gold nanoclusters
Abbreviated name: | AuNCs
Synonym:
Agent category: | Metal
Target: | Non-targeted
Target category: | Non-targeted
Method of detection: | Optical, near-infrared (NIR) fluorescence imaging
Source of signal: | Gold (Au)
Activation: | No
Studies: | - In vitro; - Rodents | No structure is currently available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=AuNCs)]

Optical fluorescence imaging is increasingly used to monitor biological functions of specific targets (1-3). However, the intrinsic fluorescence of biomolecules poses a problem when fluorophores that absorb visible light (350–700 nm) are used. Near-infrared (NIR) fluorescence (700–1,000 nm) detection avoids the background fluorescence interference of natural biomolecules, providing a high contrast between target and background tissues. NIR fluorophores have a wider dynamic range and minimal background as a result of reduced scattering compared with visible fluorescence detection. They also have high sensitivity, resulting from low infrared background, and high extinction coefficients, which provide high quantum yields. The NIR region is also compatible with solid-state optical components, such as diode lasers and silicon detectors. NIR fluorescence imaging is becoming a noninvasive alternative to radionuclide imaging in small animals (4, 5).

Gold nanoparticles have been studied as molecular imaging agents because of their bright NIR fluorescence emission around 800 nm and low toxicity (6, 7). They can be tuned to emit in a range of wavelengths by changing their sizes, shapes, and composition, thus providing broad excitation profiles and high absorption coefficients. They can be coated and capped with hydrophilic materials for additional conjugation with biomolecules, such as peptides, antibodies, nucleic acids, and small organic compounds for in vitro and in vivo studies. Gold nanoparticles are approved by the United States Food and Drug Administration for treatment of patients with rheumatoid arthritis. Gold nanoclusters (AuNCs) possess an ultrasmall size of ~2 nm compared with quantum dots (QDs, ~20 nm) (8). AuNCs are less likely to have high reticuloendothelial system accumulation. AuNCs have been studied as agents for NIR fluorescence imaging of cancerous tissues through the enhanced permeability and retention effect (9).

### Related Resource Links:

- Chapters in MICAD (Gold imaging (http://www.ncbi.nlm.nih.gov/books?term=Gold%20AND%20micad%5Bbook%5D))
- Clinical trials (Gold nanoparticles (http://www.clinicaltrials.gov/ct2/results?term=gold+AND+nanoparticles))
- Drug information in FDA (Gold nanoparticles (http://google2.fda.gov/search?q=gold%2BAND%2Brheumatoid%2Barthritis&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=9&y=12))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=AuNCs%20and%20synthesis)]

Wu et al. (9) reported the synthesis of AuNCs by addition of 0.5 ml NaOH (1 M) to a solution of 10 ml HAuCl_4_ (1 mM) containing bovine serum albumin (5 mg/ml) under vigorous stirring for 12 h at 37°C. AuNCs had a hydrodynamic diameter of 2.7 nm in phosphate-buffered saline as measured with dynamic light scattering.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=AuNCs%20and%20in%20vitro)]

AuNCs exhibited a red fluorescence emission signal (~710 nm) when excited at 465–495 nm (9). AuNCs exhibited high photostability similar to that of QDs.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=AuNCs%20and%20rodentia)]

Wu et al. (9) performed a series of whole-body NIR fluorescence imaging after intravenous injection of 0.5 mg AuNCs in normal nude mice (n = 3) and in nude mice bearing MDA-MB-45 tumors (n = 3). In normal nude mice, the fluorescence signal was immediately visualized in the superficial vasculature. AuNCs remained in the circulation at 5 h after injection. Strong fluorescence intensity was observed in the liver and urinary bladder at 1, 2, and 4 h after injection; gradual clearance was observed, but fluorescence was still visible by 24 h. Ex vivo fluorescence imaging showed that the liver had the highest signal intensity at 5 h after injection with 29% injected dose (ID)/cm^2^, followed by the kidney (18% ID/cm^2^), skin (13% ID/cm^2^), spleen (13% ID/cm^2^), intestine (11% ID/cm^2^), heart (6% ID/cm^2^), lung (5% ID/cm^2^), and muscle (4% ID/cm^2^) at the same time point. In mice bearing MDA-MB-45 tumors, fluorescence intensity in the tumor was clearly visualized at 1 h after injection, whereas signal intensity from other tissues was low. The fluorescence intensity in the tumor increased with time, with a tumor/muscle ratio of 15 at 6 h after injection. Thus, the leakiness of the tumor allows accumulation of AuNCs within the tumor by passive diffusion.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=AuNCs%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=AuNCs%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=AuNCs%20and%20human)]

No publication is currently available.

## References

1 Achilefu S. (2004). Lighting up tumors with receptor-specific optical molecular probes. Technol Cancer Res Treat.
2 Ntziachristos V., Bremer C., Weissleder R. (2003). Fluorescence imaging with near-infrared light: new technological advances that enable in vivo molecular imaging. Eur Radiol.
3 Becker A., Hessenius C., Licha K., Ebert B., Sukowski U., Semmler W., Wiedenmann B., Grotzinger C. (2001). Receptor-targeted optical imaging of tumors with near-infrared fluorescent ligands. Nat Biotechnol.
4 Ke S., Wen X., Gurfinkel M., Charnsangavej C., Wallace S., Sevick-Muraca E.M., Li C. (2003). Near-infrared optical imaging of epidermal growth factor receptor in breast cancer xenografts. Cancer Res.
5 Tung C.H. (2004). Fluorescent peptide probes for in vivo diagnostic imaging. Biopolymers.
6 Vosch T., Antoku Y., Hsiang J.C., Richards C.I., Gonzalez J.I., Dickson R.M. (2007). Strongly emissive individual DNA-encapsulated Ag nanoclusters as single-molecule fluorophores. Proc Natl Acad Sci U S A.
7 Chithrani B.D., Ghazani A.A., Chan W.C. (2006). Determining the size and shape dependence of gold nanoparticle uptake into mammalian cells. Nano Lett.
8 Shang, L., R.M. Dorlich, S. Brandholt, R. Schneider, V. Trouillet, M. Bruns, D. Gerthsen, and G.U. Nienhaus, Facile preparation of water-soluble fluorescent gold nanoclusters for cellular imaging applications. Nanoscale, 2011
9 Wu X., He X., Wang K., Xie C., Zhou B., Qing Z. (2010). Ultrasmall near-infrared gold nanoclusters for tumor fluorescence imaging in vivo. Nanoscale.